# Polyethylene glycol–coated (PEG5000) gold nanoparticles

Chemical name: | Polyethylene glycol–coated (PEG5000) gold nanoparticles
Abbreviated name: | PEGylated gold nanoparticles
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Ultrasound, Photoacoustic Imaging (PAI)
Source of signal / contrast: | Gold (Au)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=photoacoustic+imaging)]

Gold nanoparticles belong to a small class of nanomaterials, while have been intensively investigated for biomedical use because of their excellent biocompatibility with human tissues and high affinity for functional groups such as thiols, phosphines, and amines (1-5). Gold nanoparticles have been approved by the United States Food and Drug Administration to treat human rheumatoid arthritis. They also have been used to enhance tumor sensitivity to radiation therapy. Surface-enhanced Raman scattering of gold nanoparticles has been tested for optical imaging of tumors (1, 6). Gold and gold-speckled silica nanoparticles have recently been developed as contrast agents for photoacoustic imaging (PAI) and multimodality imaging (3, 5, 7).

Gold nanoparticles for PAI are based on either surface plasmon resonance (SPR) or fluorescent dyes attached to or encapsulated within nanoparticles. Nanoshells and nanorods are two representatives of SPR-based contrast agents (1, 7, 8). Peak absorption can be tuned throughout the visible and near-infrared (NIR) regions by controlling the physical dimensions of the metallic layer of nanoshells and the cylindrical symmetry of nanorods. Both nanoshells and nanorods exhibit good resistance to chemical/thermal denaturation and photobleaching. Dye-doped NIR nanoparticles function on the basis of strong optical absorption in the NIR region (3). Furthermore, dye encapsulation in nanoparticles significantly increases the circulation time of dyes in blood, allowing for extended imaging periods. On the other hand, proper comparison among nanoparticles appears difficult because shapes, sizes, materials, and mechanisms of different nanoparticles vary.

Cai et al. reported the feasibility of gold nanoparticles modified with a methoxy-polyethylene glycol (PEG) sulhydryl moiety (molecular weight: 2.0 kDa) as a contrast agent for X-ray and computed tomography (MICAD chapter on PEG-AuNPs (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Au-PEG-NP)) (9). Recently, Zhang et al. modified gold nanoparticles with a PEG5000-thiol moiety and tested the PEGylated nanoparticles as a PAI contrast agent in vivo (5). Zhang et al. demonstrated the ability of PEGylated gold nanoparticles to detect tumors in vivo with photoacoustic tomography (PAT) (5). Their findings also suggest an opportunity for image-guided cancer therapy, with non-targeted gold nanoparticles serving as tumor-imaging contrast agents and mediators of cancer therapy.

### Related Resource Links:

MICAD chapters on gold nanoparticles for imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=gold+nanoparticles+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

Clinical trials of gold products in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=gold)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19726840)]

Zhang et al. synthesized the gold nanoparticles with citrate reduction of auric chloride (HAuCl_4_) (5). The sizes of gold nanoparticles (20-nm and 50-nm nanoparticles were used in the experiments) were controlled by changing the concentration of citrate with respect to HAuCl_4_ (10). The generated gold particles were separated with centrifugation, followed by modification with PEG5000-thiol to obtain PEGylated nanoparticles (~4–5 PEG molecules/nm^2^ gold surface area). The measured sizes of final nanoparticles were ~52 nm and ~20 nm, respectively, with a polydispersity index of 1.08. The PEGylation reaction did not result in any significant variation for the nanoparticle sizes. The maximum optical absorption was ~525 nm and 530 nm for 20-nm and 50-nm nanoparticles, respectively, and the absorption coefficient at 532 nm was 0.018 mm^-1^ and 0.025 mm^-1^ for 20-nm and 50-nm nanoparticles, respectively. The yield, purity, and number of PEG per particle for the nanoparticles were not described (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19726840)]

Light-induced acoustic signal was assessed with mouse skin and 50-nm nanoparticles embedded separately 2 mm deep in a phantom (5). The phantom was constructed with 1% intralipid india ink, distilled water, and 2% agar power. The absorption and scattering coefficients of the phantom at 532 nm were 0.007 mm^-1^ and 1.0 mm^-1^, respectively. After illumination with a pulsed laser beam, both skin (5 mm x 4 mm) and nanoparticles were clearly imaged with PAT, and the reconstructed sizes of skin and nanoparticles were very close to their actual sizes. The optical absorption of nanoparticles was 1.6 (arbitrary units), 3.2-fold higher than that of skin (0.5 units).

Light-induced acoustic signal was further assessed with injection of the gold nanoparticles (50 nm) into the mouse skin, and the skin implanted in a phantom (5). Images clearly showed the approximate shape of the skin. The optical absorption of the skin with nanoparticles was 0.70 units, while that of the skin region without nanoparticles was 0.40 units. There was a contrast of 1.8 between the skin regions with and without nanoparticles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19726840)]

In vivo PAT was performed before and after injection of 20-nm and 50-nm gold nanoparticles into the subcutaneous abdominal wall of C57/BL6 mice. Both types of nanoparticles were clearly imaged with excellent contrast (5). The saline control showed little change in absorption.

In vivo tumor PAT was carried out after administration of 50-nm nanoparticles via the tail vein of mice bearing BT474 breast cancer xenografts. Accumulation of the gold nanoparticles in tumors was observed clearly with PAT at 5 h after administration. Subtraction of the data at 3 h from the absorption at 5 h showed significant enhancement in the signal intensity over this time period, indicating an accumulation of the nanoparticles over time in the tumor region due to the enhanced permeability and retention effect.

The investigators declared that a direct comparison between 20-nm and 50-nm nanoparticles in vivo was difficult because multiple factors, including intratumoral distribution of particles, delivery, metabolism, and depth of injection, could contribute to the observed signal intensity (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Yang X., Stein E.W., Ashkenazi S., Wang L.V. (2009). Nanoparticles for photoacoustic imaging. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
2 Copland J.A., Eghtedari M., Popov V.L., Kotov N., Mamedova N., Motamedi M., Oraevsky A.A. (2004). Bioconjugated gold nanoparticles as a molecular based contrast agent: implications for imaging of deep tumors using optoacoustic tomography. Mol Imaging Biol.
3 de la Zerda A., Liu Z., Bodapati S., Teed R., Vaithilingam S., Khuri-Yakub B.T., Chen X., Dai H., Gambhir S.S. (2010). Ultrahigh sensitivity carbon nanotube agents for photoacoustic molecular imaging in living mice. Nano Lett.
4 Wang L.V. (2008). Prospects of photoacoustic tomography. Med Phys.
5 Zhang Q., Iwakuma N., Sharma P., Moudgil B.M., Wu C., McNeill J., Jiang H., Grobmyer S.R. (2009). Gold nanoparticles as a contrast agent for in vivo tumor imaging with photoacoustic tomography. Nanotechnology.
6 Hainfeld J.F., Slatkin D.N., Smilowitz H.M. (2004). The use of gold nanoparticles to enhance radiotherapy in mice. Phys Med Biol.
7 Sharma P., Brown S.C., Bengtsson N., Zhang Q., Walter G.A., Grobmyer S.R., Santra S., Jiang H., Scott E.W., Moudgil B.M. (2008). Gold-Speckled Multimodal Nanoparticles for Noninvasive Bioimaging. Chem Mater.
8 Yang X., Skrabalak S.E., Li Z.Y., Xia Y., Wang L.V. (2007). Photoacoustic tomography of a rat cerebral cortex in vivo with au nanocages as an optical contrast agent. Nano Lett.
9 Cai Q.Y., Kim S.H., Choi K.S., Kim S.Y., Byun S.J., Kim K.W., Park S.H., Juhng S.K., Yoon K.H. (2007). Colloidal gold nanoparticles as a blood-pool contrast agent for X-ray computed tomography in mice. Invest Radiol.
10 Ji X., Song X., Li J., Bai Y., Yang W., Peng X. (2007). Size control of gold nanocrystals in citrate reduction: the third role of citrate. J Am Chem Soc.